# 3-Chloro-4-[^18^F]fluorophenyl-(4-fluoro-4-[[(5-methyl-pyrimidin-2-ylmethyl)-amino]-methyl]-piperidin-1-yl)methanone (F15599)

Chemical name: | 3-Chloro-4-[^18^F]fluorophenyl-(4-fluoro-4-[[(5-methyl-pyrimidin-2-ylmethyl)-amino]-methyl]-piperidin-1-yl)methanone (F15599)
Abbreviated name: | [^18^F]F15599
Synonym:
Agent category: | Compound
Target: | 5-HT_1A_ serotonin receptor
Target category: | Receptor
Method of detection: | Positron emission tomography (PET)
Source of signal: | ^18^F
Activation: | No
Studies: | - In vitro; - Rodents; - Non-primate non-rodent mammals | Click on the above structure for additional information in PubChem (http://pubchem.ncbi.nlm.nih.gov/).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=F15599)]

5-Hydroxytryptamine (5-HT), commonly known as serotonin, has diverse physiological roles as a neurotransmitter in the central nervous system (1). 5-HT is involved in regulation and modulation of sleep, affective and personality behaviors, and pain. It also is a regulator of smooth muscle function and platelet aggregation. The brain cortical 5-HT system has been implicated in several neuropsychiatric disorders, including major depression, anxiety, schizophrenia, and obsessive-compulsive disorder (2, 3). The effects of 5-HT are mediated by as many as seven classes of receptor populations (5-HT_1_ to 5-HT_7_), many of which include several subtypes (4). There are five receptor subtypes within the G-protein–coupled 5-HT_1_ receptor family: 5-HT_1A_, 5-HT_1B_, 5-HT_1D_, 5-HT_1E_, and 5-HT_1F_.

5-HT_1A_ receptors are abundantly present in the hippocampus, entorhinal cortex, frontal cortex, raphe nucleus, and septum; the lowest densities are observed in the basal ganglia, substantia nigra, and cerebellum (5). Some thalamic and hypothalamic nuclei have intermediate densities. 5-HT_1A_ receptors are involved in the mediation of emotion and the function of the hypothalamus. 5-HT_1A_ receptors are implicated in anxiety, depression, hallucinogenic behavior, motion sickness, and eating disorders (6). Thus, there is a need for selective ligands to investigate the pharmacological role of 5-HT_1A_ receptors.

There have been several studies to develop specific 5-HT_1A_ radioligands [PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=5-HT1a%5BAll%20Fields%5D%20AND%20imaging%5BAll%20Fields%5D)] for positron emission tomography (PET) imaging, such as [carbonyl-^11^C]WAY 100635 (http://www.ncbi.nlm.nih.gov/books/NBK23263/), [^18^F]FPWAY (http://www.ncbi.nlm.nih.gov/books/NBK23137/), and [^18^F]MPPF (http://www.ncbi.nlm.nih.gov/books/NBK23391/). However, none of these antagonists distinguishes between the high- and low-affinity states of the 5-HT_1A_ receptors. The high-affinity state of the receptor is coupled to G-proteins, which mediate cell functions by providing intracellular signals. 2-(4-(4-(2-Methoxyphenyl)piperazin-1-yl)butyl)-4-methyl-1,2,4-triazine-3,5(2H,4H)dione (MMP) was reported to be a potent agonist of 5-HT_1A_ receptors (K_i_ = 0.15 nM) (7). This led to the development of [O-methyl-^11^C]MMP([^11^C]MMP (http://www.ncbi.nlm.nih.gov/books/NBK23229/), also known as [^11^C]CUMI-101) as a useful tool for in vivo PET imaging of the 5-HT_1A_ receptor (8-10). However, [^11^C]CUMI-101 was shown to be a partial 5-HT_1A_ agonist and therefore was less efficient in mediating cell function (11, 12). 3-Chloro-4-[^18^F]fluorophenyl-(4-fluoro-4-[[(5-methyl-pyrimidin-2-ylmethyl)-amino]-methyl]-piperidin-1-yl)methanone ([^18^F]F15599) was evaluated as a PET probe for the 5-HT_1A_ receptor (13) because unlabeled F15599 was found to be a selective 5-HT_1A_ agonist with nanomolar affinity for the 5-HT_1A_ receptor (14).

### Related Resource Links:

- Chapters in MICAD (5-HT_1A_ (http://www.ncbi.nlm.nih.gov/sites/entrez?db=Books&cmd=Search&term=5-HT1A+AND+micad%5bbook%5d&doptcmdl=TOCView&log%24=booksrch&bname=micad))
- Gene information in NCBI (5-HT_1A_ (http://www.ncbi.nlm.nih.gov/gene/3350))
- Articles in Online Mendelian Inheritance in Man (OMIM) (5-HT_1A_ (http://www.ncbi.nlm.nih.gov/omim/109760))
- Clinical trials (5-HT_1A_ (http://www.clinicaltrials.gov/ct2/results?term=5-HT1A))
- Drug information in Food and Drug Administration (5-HT_1A_ (http://google2.fda.gov/search?q=5-HT1a&client=FDAgov&site=FDAgov&lr=&proxystylesheet=FDAgov&output=xml_no_dtd&getfields=*&x=8&y=1))

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=F15599%20and%20synthesis)]

The automated radiosynthesis of [^18^F]F15599, reported by Lemoine et al. (13), involved standard fluoronucleophilic substitution of the corresponding nitro precursor with K[^18^F]F/Kryptofix2.2.2 in dimethyl sulfoxide for 30 min at 150°C in an automated radiosynthesis unit, followed by solid-phase extraction with a C18 cartridge. The reported overall radiochemical yield of the radiosynthesis was ~30%, the specific activity was 85–120 MBq/nmol (2.3–3.2 mCi/nmol) at the end of synthesis (EOS), and the radiochemical purity was >98%. The total synthesis time was 80 min. The log P value for [^18^F]F15599 was 1.17 (lipophilic).

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=F15599%20and%20in%20vitro)]

Lemoine et al. (13) performed in vitro autoradiography with [^18^F]F15599 in rat and cat brains, which showed radioactivity in the cingulate, hippocampus, and raphe nucleus. Little radioactivity was observed in the cerebellum, a region poor in 5-HT_1A_ receptors. In comparison with [^18^F]MPPF (a 5-HT_1A_ antagonist), the radioactivity levels of [^18^F]F15599 were 50%–80% less than those of [^18^F]MPPF in the hippocampus and raphe nucleus in both rats and cats. Competition binding studies of WAY100635 (a 5-HT_1A_ antagonist) and 8-OH-DPAT (a 5-HT_1A_ agonist) with [^18^F]F15599 in rat hippocampus sections were also performed. WAY100635 reduced the binding of [^18^F]F15599 by 69% and 76% with 10 nM and 100 nM WAY100635, respectively. 8-OH-DPAT inhibited the binding by 67% and 85% with 10 nM and 100 nM 8-OH-DPAT, respectively. Gpp(NH)p (10 µM, a non-hydrolysable analog of guanosine 5'-triphosphate) inhibited the [^18^F]F15599 binding by 70% in the hippocampus (P < 0.05).

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=F15599%20and%20rodentia)]

Ex vivo stability studies (n = 3/group) of [^18^F]F15599 in rat brain hippocampus were performed after intravenous injection of 55.5 MBq (1.5 mCi) [^18^F]F15599 (13). [^18^F]F15599 remained 80%, 90%, 97%, and 85% intact in the brain at 10, 20, 30, and 40 min after injection, respectively.

Ex vivo PET imaging studies (n = 3/group) were performed in the excised rat brains at 30 min after injection of 74 MBq (2 mCi) [^18^F]F15599 (13). Higher radioactivity levels were observed in the cingulate cortex and hippocampus than in the striatum and cerebellum. Pretreatment or post-treatment with excess WAY100635 decreased [^18^F]F15599 binding in the cortical areas, whereas no reduction of radioactivity levels was observed in the cerebellum. In vivo PET imaging studies were also performed. High radioactivity levels were observed in the hippocampus and cingulate cortex. The cingulate cortex/cerebellum and hippocampus/cerebellum ratios were 1.6 and 1.2, respectively.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=F15599%20and%20%28dog%20or%20pig%20or%20sheep%20or%20rabbit%29)]

Lemoine et al. (13) performed in vivo PET imaging studies in the brain of one male cat for 90 min after injection of 74 MBq (2 mCi) [^18^F]F15599. High radioactivity levels were observed in the raphe nucleus, cingulate cortex, and amygdala. The cingulate cortex/cerebellum, amygdala/cerebellum, and raphe nucleus/cerebellum ratios were 1.3, 1.3, and 1.5, respectively.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=F15599%20and%20nonhuman%20primate)]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=F15599%20and%20human)]

No publication is currently available.

## References

1 Lucki I. (1998). The spectrum of behaviors influenced by serotonin. Biol Psychiatry.
2 Fletcher A., Cliffe I.A., Dourish C.T. (1993). Silent 5-HT1A receptor antagonists: utility as research tools and therapeutic agents. Trends Pharmacol Sci.
3 Hoyer D., Clarke D.E., Fozard J.R., Hartig P.R., Martin G.R., Mylecharane E.J., Saxena P.R., Humphrey P.P. (1994). International Union of Pharmacology classification of receptors for 5-hydroxytryptamine (Serotonin). Pharmacol Rev.
4 Lanfumey L., Hamon M. (2004). 5-HT1 receptors. Curr Drug Targets CNS Neurol Disord.
5 Pazos A., Probst A., Palacios J.M. (1987). Serotonin receptors in the human brain--III. Autoradiographic mapping of serotonin-1 receptors. Neuroscience.
6 Cowen P.J. (2000). Psychopharmacology of 5-HT(1A) receptors. Nucl Med Biol.
7 Kumar J.S., Prabhakaran J., Majo V.J., Milak M.S., Hsiung S.C., Tamir H., Simpson N.R., Van Heertum R.L., Mann J.J., Parsey R.V. (2007). Synthesis and in vivo evaluation of a novel 5-HT(1A) receptor agonist radioligand [O-methyl- (11)C]2-(4-(4-(2-methoxyphenyl)piperazin-1-yl)butyl)-4-methyl-1,2,4-triazi ne-3,5(2H,4H)dione in nonhuman primates. Eur J Nucl Med Mol Imaging.
8 Milak M.S., Severance A.J., Prabhakaran J., Kumar J.S., Majo V.J., Ogden R.T., Mann J.J., Parsey R.V. (2011). In vivo serotonin-sensitive binding of [11C]CUMI-101: a serotonin 1A receptor agonist positron emission tomography radiotracer. J Cereb Blood Flow Metab.
9 Hines C.S., Liow J.S., Zanotti-Fregonara P., Hirvonen J., Morse C., Pike V.W., Innis R.B. (2011). Human biodistribution and dosimetry of (1)(1)C-CUMI-101, an agonist radioligand for serotonin-1a receptors in brain. PLoS One.
10 Milak M.S., DeLorenzo C., Zanderigo F., Prabhakaran J., Kumar J.S., Majo V.J., Mann J.J., Parsey R.V. (2010). In vivo quantification of human serotonin 1A receptor using 11C-CUMI-101, an agonist PET radiotracer. J Nucl Med.
11 Hendry N., Christie I., Rabiner E.A., Laruelle M., Watson J. (2011). In vitro assessment of the agonist properties of the novel 5-HT1A receptor ligand, CUMI-101 (MMP), in rat brain tissue. Nucl Med Biol.
12 Palner M., Underwood M.D., Kumar D.J., Arango V., Knudsen G.M., John Mann J., Parsey R.V. (2011). Ex vivo evaluation of the serotonin 1A receptor partial agonist [(3)H]CUMI-101 in awake rats. Synapse.
13 Lemoine L., Verdurand M., Vacher B., Blanc E., Le Bars D., Newman-Tancredi A., Zimmer L. (2010). [18F]F15599, a novel 5-HT1A receptor agonist, as a radioligand for PET neuroimaging. Eur J Nucl Med Mol Imaging.
14 Maurel J.L., Autin J.M., Funes P., Newman-Tancredi A., Colpaert F., Vacher B. (2007). High-efficacy 5-HT1A agonists for antidepressant treatment: a renewed opportunity. J Med Chem.